# ^99m^Tc-Hydrazinonicotinic acid-cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Met-Phe-NH_2_

Chemical name: | ^99m^Tc-Hydrazinonicotinic acid-cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Met-Phe-NH_2_
Abbreviated name: | ^99m^Tc-HYNIC-cyclo-MG1
Synonym:
Agent category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2) receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); planar gamma imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=417029), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=33356159) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the CCK2 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+gastrin+analogs)]

The gastrointestinal peptides gastrin and cholecystokinin-2 (CCK2) have various regulatory functions in the brain and gastrointestinal tract (1). Both peptides have the same COOH-terminal pentapeptide amide sequence, GWMDF-NH_2_, which is the biologically active site (2). Human gastrin is a peptide composed of 33 amino acids and also exists in several C-terminal–truncated forms (3). These truncated forms include minigastrin (MG0), which is a 13-residue peptide with the sequence of D-Glu-Glu-Glu-Glu-Glu-Glu-Ala-Tyr-Gly-Trp-Met-Asp-Phe-NH_2_. CCKs exist in a variety of biologically active molecular fragments ranging from 4 to 18 amino acids, including sulphated and unsulphated CCK8, which is an octapeptide (Asp-Tyr-Met-Gly-Trp-Met-Asp-Phe-NH_2_) (4). Two CCK receptor subtypes have been identified in normal tissues by their binding affinities to gastrin. CCK1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK2 (CCK-B, brain) receptors have high affinity for gastrin (4). The sulphated CCK8 peptide displays high affinity for both CCK1 and CCK2 receptors, which are G-protein–coupled (5). These receptors have also been found to be overexpressed in a variety of tumor types (5). CCK2 receptors have been found most frequently in medullary thyroid carcinomas, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (1). CCK1 receptors have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastomas. Radiolabeled CCK8 peptides have been studied in tumors expressing CCK2 receptors with good specificity for potential in vivo imaging.

A cyclized minigastrin analog, cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Met-Phe-NH_2_ (cyclo-MG1), for the gastrin receptor was N-terminally conjugated with hydrazinonicotinic acid (HYNIC) for radiolabeling with ^99m^Tc and ethylenediamine-N,N’-diacetic acid (EDDA) as a coligand to form ^99m^Tc-HYNIC-cyclo-MG1 (6), which has been evaluated for imaging tumors expressing CCK2 receptors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=cholecystokinin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Gastrin/cholecystokinin-2 receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=118444)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cyclo-MG1)]

Cyclo-MG1 was prepared by solid-phase peptide synthesis (6). The N-terminus was conjugated with a HYNIC-chelating group to produce HYNIC-cyclo-MG1 by N-hydroxysuccinimidyl-HYNIC. HYNIC-MG1 was purified with reverse-phase high-performance liquid chromatography. Radiolabeling was performed by mixing HYNIC-cyclo-MG1 (10-20 µg) with an EDDA/tricine solution, 400 MBq Na^99m^TcO_4_, and ZnCl_2_ (pH 6). The mixture was heated for 30 min at 100°C. The radiochemical purity and specific activity of ^99m^Tc-HYNIC-cyclo-MG1 were >90% and 20–60 TBq/mmol (540–1,620 Ci/mmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cyclo-MG1+and+in+vitro)]

An in vitro receptor-binding assay of ^99m^Tc-HYNIC-cyclo-MG1 was performed on CCK2 receptor–expressing AR42J cells with an affinity constant (K_d_) of 19.1 nM (6). Binding of ^99m^Tc-HYNIC-cyclo-MG1 to AR42J cells was 93.5 ± 1.1% of the incubation dose after 120 min at 37°C. ^99m^Tc-HYNIC-cyclo-MG1 exhibited high stability (94–98% intact) in a phosphate-buffered solution containing excess cysteine and human plasma after 24 h of incubation. Log P_7.4_ of ^99m^Tc-HYNIC-cyclo-MG1 was -3.01.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cyclo-MG1+and+rodentia)]

Von Guggenberg et al. (6) performed ex vivo biodistribution studies of ^99m^Tc-HYNIC-cyclo-MG1 in nude mice (n = 3/group) bearing R42J tumor xenografts. Each mouse received 1 MBq (27 nCi) ^99m^Tc-HYNIC-cyclo-MG1 by intravenous injection. The tumor radioactivity levels were 3.61 ± 0.40% injected dose per gram (ID/g) at 1 h and 3.40 ± 0.69% ID/g at 4 h. The accumulation of radioactivity in the tumor was blocked by excess human minigastrin to 1.46 ± 0.71% ID/g at 1 h after co-injection. The kidney radioactivity levels (1.92% ID/g at 1 h and 1.95% ID/g at 4 h) were not blocked by human minigastrin. The blood, lung, heart, spleen, pancreas, and liver radioactivity levels were <0.4% ID/g at these two time points. The intestine and stomach radioactivity levels at 1 h were 1.79 ± 0.36 and 1.15 ± 0.39% ID/g, respectively. Accumulation in the intestine and stomach was slightly blocked by human minigastrin to 1.37 ± 0.09 and 0.86 ± 0.32% ID/g, respectively. Little inhibition of radioactivity was observed in the other tissues. The tumor/blood and tumor/muscle ratios were 15 and 36 at 1 h, respectively. The tumor, abdominal area, and kidneys were clearly visualized with single-photon emission computed tomography scintigraphy imaging at 1 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cyclo-MG1+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cyclo-MG1+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cyclo-MG1+and+human)]

No publication is currently available.

## References

1 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
2 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
3 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
4 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
5 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
6 von Guggenberg E., Sallegger W., Helbok A., Ocak M., King R., Mather S.J., Decristoforo C. (2009). Cyclic minigastrin analogues for gastrin receptor scintigraphy with technetium-99m: preclinical evaluation. J Med Chem.